# 2-{[4-(4-[^125^I]Iodobenzyl)piperidin-1-yl]methyl}benzimidazol-5-ol

Chemical name: | 2-{[4-(4-[^125^I]Iodobenzyl)piperidin-1-yl]methyl}benzimidazol-5-ol
Abbreviated name: | [^125^I]8
Synonym:
Agent Category: | Compound
Target: | N-methyl-D-aspartate (NMDA) receptor
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information on [^125^I]8 in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Functions%20of%20NMDA%20receptor&cmd=DetailsSearch)]

The N-methyl-D-aspartate (NMDA) receptor (NMDAR) belongs to a sub-group of the glutamate receptor family and has a heteromeric structure that is made up of three subunits (NR1, NR2, and NR3) as dimeric combinations (NR1/NR2 or NR1/NR3). There are four subtypes of NR2 (NR2A–NR2D), and NR3 has two subtypes, NR3A and NR3B. The NMDAR can bind several different types of ligands and has important functions in the process of learning and in the performance of memory tasks in a variety of animal species (invertebrate and vertebrate) (1, 2). These receptors are involved in the development of neurological conditions such as Parkinson’s disease, Alzheimer’s disease, bipolar disorder, etc (2, 3). The structure, distribution, and function of the NMDAR in the rodent brain has been reviewed elsewhere (1, 4). The NR1 subunit of the NMDAR is known to be distributed in all parts of the brain; of the different NR2 subtypes, NR2A is found throughout the brain, whereas NR2B, NR2C, and NR2D are present mainly in the forebrain (including the cerebral cortex, hippocampus, and the olfactory lobes), cerebellum, and the lower brain stem, respectively. High levels of the NR3A subtype are detected in many brain regions of only prenatal and newborn mice, whereas NR3B levels are low during these developmental stages. However, the NR3 subtype is expressed predominantly in the adult brain (4).

Among the different NR2 and NR3 subunits, primarily the NR2B subunit is believed to modulate the various physiological and pharmacological activities of the NMDAR as mentioned above. Attempts to study the distribution of the NMDAR that contains the NR2B subunit in the brain through the use of positron emission tomography with radiolabeled compounds have been unsuccessful because the tracers lack binding specificity for the receptor (3). However, among these tracers, the uptake of 6-{3-[4-(4-fluorobenzyl)piperidino]propionyl}-3H-benzoxazol-2-[^11^C]-one ([^11^C]EMD-95885; a benzimidazole derivative) in the rodent brain was reduced by pretreatment of the animals with ifenprodil, a selective antagonist of the NR2B subunit, suggesting that [^11^C]EMD-95885 could be a suitable platform for the development of new imaging probes to study the location and distribution of NMDARs that contain the NR2B subunit in the rodent brain (3). Results from in vitro assays demonstrated that novel compounds with a structure resembling EMD-95885 maintained their affinity for the NR2B subunit (5). On the basis of this information, Fuchigami et al. synthesized a series of ^125^I-labeled benzimidazole derivatives and investigated their in vitro receptor binding and in vivo brain uptake characteristics in normal mice (3). Among these radioiodinated compounds, only two, 2-{[4-(4-[^125^I]iodobenzyl) piperidin-1-yl]methyl}benzimidazol-5-ol ([^125^I]8) and N-{2-[4-(4-[^125^I]iodobenzyl)-piperidin-1-ylmethyl]benzoimidazol-5-yl}-methanesulfonamide ([^125^I]9), were shown to have a high affinity for the NR2B subunit under in vitro conditions. This chapter discusses the in vitro and in vivo results obtained with [^125^I]8; the characteristics of [^125^I]9 are described in a separate chapter of MICAD (www.micad.nih.gov) (6).

### Other Sources of Information

Other chapters on NMDAR in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=NMDA%20receptor%20AND%20micad%5Bbook%5D)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001177656.1) of NMDA1 receptor (zeta 1) (Grin1), transcript variant 2

Information regarding NMDAR on FDA site (http://google2.fda.gov/search?q=NMDA+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=12)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=NMDA+receptor) on NMDAR

NR2A subunit (http://www.ncbi.nlm.nih.gov/omim/138253) in OMIM (Online Mendelian Inheritance in Man)

NR2B subunit (http://www.ncbi.nlm.nih.gov/omim/138252) in OMIM (Online Mendelian Inheritance in Man)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-%7B%5B4-%284-%5B125I%5DIodobenzyl%29piperidin-1-yl%5Dmethyl%7Dbenzimidazol-5-ol%20synthesis&cmd=DetailsSearch)]

The synthesis of [^125^I]8 has been detailed by Fuchigami et al. (3). The radiochemical yield of [^125^I]8 was reported to be 85%–90% based on the amount of [^125^I]sodium iodide used in the synthesis. The radiochemical purity of the final product was >98% as determined with high-performance liquid chromatography. The specific activity and in vitro stability of [^125^I]8 were not reported.

Using the shake-flask method, the partition coefficient of 8 between octanol and phosphate-buffered saline (pH 7.4) was determined to be 3.95 (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-%7B%5B4-%284-%5B125I%5DIodobenzyl%29piperidin-1-yl%5Dmethyl%7Dbenzimidazol-5-ol%20in%20vitro&cmd=DetailsSearch)]

Using an in vitro [^3^H]ifenprodil displacement assay with rat cortical membrane homogenates, the K_i_ of 8 was determined to be 7.28 ± 2.93 nM (3).

In another study, the distribution of [^125^I]8 in rat brain sections was investigated with an autoradiographic technique as described elsewhere (3). Radioiodinated 8 accumulated primarily in the forebrain (cerebral cortex and hippocampus; these regions are rich in NR2B), but a low level of the tracer was detected in the cerebellum, which exhibits low expression of NR2B. In general, the tracer showed a high non-specific binding in the brain sections. Pretreatment of the brain sections with Ro-25,6981, an NR2B-selective anatagonist, was shown to inhibit the binding of [^125^I]8 in the different parts of the forebrain, indicating that the tracer probably had some specificity for the NR2B subunit of the NMDAR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-%7B%5B4-%284-%5B125I%5DIodobenzyl%29piperidin-1-yl%5Dmethyl%7Dbenzimidazol-5-ol%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^125^I]8 was investigated in normal ddY mice (n = 5–6 animals per time point) as described by Fuchigami et al. (3). The animals were injected with the tracer through the tail vein and euthanized at predetermined time points to measure the amount of radioactivity that accumulated in the major organs. Data were presented as percent injected dose per gram tissue (% ID/g). Maximum uptake of the radioiodinated compound was observed in the liver. Accumulation in the liver was 25.03 ± 4.20% ID/g at 5 min postinjection (p.i.), increased to 32.22 ± 6.56% ID/g at 180 min p.i., and remained relatively constant up to 360 min p.i. In the kidneys, the accumulation was 12.20 ± 3.18% ID/g at 5 min p.i. and decreased to 5.46 ± 0.67% ID/g at 360 min p.i. The lungs showed an uptake of 14.48 ± 2.52% ID/g at 5 min p.i., which decreased to 3.44 ± 0.80% ID/g at 360 p.i. Accumulation in the brain was 0.42 ± 0.06% ID/g at 5 min p.i. and increased to 0.55 ± 0.14% ID/g at 360 min p.i. The brain/blood (B/B) ratio for [^125^I]8 increased from 0.36 ± 0.03 at 5 min p.i. to 0.67 ± 0.12 at 30 min p.i. and to 2.23 ± 0.99 at 360 min p.i.

To confirm the binding specificity of [^125^I]8 in different regions of the brain, blocking studies were performed by the administration of unlabeled 8 or Ro-25,6981 (3 mg/kg body weight) to the animals (n = 5 mice/blocking drug) 30 min before injecting the labeled compound (3). The animals were euthanized at 180 min p.i., and the brains were removed to determine the amount of radioactivity accumulated in the cerebral cortex, hippocampus, and cerebellum. Animals pretreated with the blocking drugs were reported to have markedly lower (P < 0.01) cerebral cortex/blood (~0.4 and ~0.6 for 8 and Ro-25,6981, respectively), hippocampus/blood (~0.4 and ~0.6 for 8 and Ro-25,6981, respectively), and the cerebellum/blood (~0.4 and ~0.6 for 8 and Ro-25,6981, respectively) ratios compared to controls (~1.0 for each brain area). This indicated that [^125^I]8 probably had a binding specificity for the NMDAR that contains the NR2B subtype subunit On the basis of observations that there was a low, uniform uptake of [^125^I]8 in almost all regions of the rodent brain and little evidence that it bound specifically to the NMDAR that contains the NR2B subunit the investigators concluded that this radioiodinated compound was probably not suitable for single-photon emission computed tomography imaging of the cerebral NMDAR.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-%7B%5B4-%284-%5B125I%5DIodobenzyl%29piperidin-1-yl%5Dmethyl%7Dbenzimidazol-5-ol%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-%7B%5B4-%284-%5B125I%5DIodobenzyl%29piperidin-1-yl%5Dmethyl%7Dbenzimidazol-5-ol%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=2-%7B%5B4-%284-%5B125I%5DIodobenzyl%29piperidin-1-yl%5Dmethyl%7Dbenzimidazol-5-ol%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Magnusson K.R., Brim B.L., Das S.R. (2010). Selective Vulnerabilities of N-methyl-D-aspartate (NMDA) Receptors During Brain Aging. Front Aging Neurosci.
2 Teng H., Cai W., Zhou L., Zhang J., Liu Q., Wang Y., Dai W., Zhao M., Sun Z. (2010). Evolutionary mode and functional divergence of vertebrate NMDA receptor subunit 2 genes. PLoS One.
3 Fuchigami T., Yamaguchi H., Ogawa M., Biao L., Nakayama M., Haratake M., Magata Y. (2010). Synthesis and biological evaluation of radio-iodinated benzimidazoles as SPECT imaging agents for NR2B subtype of NMDA receptor. Bioorg Med Chem.
4 Low C.M., Wee K.S. (2010). New insights into the not-so-new NR3 subunits of N-methyl-D-aspartate receptor: localization, structure, and function. Mol Pharmacol.
5 Borza I., Kolok S., Gere A., Nagy J., Fodor L., Galgoczy K., Fetter J., Bertha F., Agai B., Horvath C., Farkas S., Domany G. (2006). Benzimidazole-2-carboxamides as novel NR2B selective NMDA receptor antagonists. Bioorg Med Chem Lett.
6 Chopra, A., N-{2-[4-(4-[125I]iodobenzyl)-piperidin-1-ylmethyl]benzoimidazol-5-yl}-methanesulfonamide. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.